# Cy5.5-CGRRRQRRKKRG-Labeled T lymphocytes

Chemical name: | Cy5.5-CGRRRQRRKKRG-Labeled T lymphocytes
Abbreviated name: | Cy5.5-Tat-T cells
Synonym:
Agent category: | Labeled cell
Target: | Other
Target category: | Other –inflamed tissue
Method of detection: | Near-infrared fluorescence (NIRF) optical imaging
Source of signal/contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5 + TAT + T cell)]

T cells are responsible for regulating immune responses and maintaining immune tolerance via recognition of peptide antigens that are bound to human leukocytes (1). Some T cells possess autoimmunity or self-tolerance through recognition of self-antigens. Loss of this required self-tolerance can result in an autoimmune disorder. For instance, experimental allergic encephalomyelitis (EAE) is one of immune-mediated diseases in which immune cells become reactive against myelins, which leads to the destruction of myelin sheets (2). EAE can be induced in rodents by adoptive transfer of CD4^+^ T cells specific to myelin basic protein (MBP), an autoantigen of myelin (3). As an animal model for the inflammatory disease, EAE can reproduce many clinical neuropathological and immunological aspects of multiple sclerosis (MS) and thus has been widely used in therapeutic development for MS (4). The evolution of inflammatory lesions in EAE involves several steps (1, 3). After intravenous administration, the injected MBP-specific T cells cross the blood–brain barrier to recognize the T cell antigen located on perivascular microglia. This antigen-specific interaction produces a plethora of inflammatory cytokines and mediators, leading to amplification of the inflammatory reaction. The blood–brain barrier then opens to allow antigen-independent recruitment of various mononuclear inflammatory cells into the central nervous system, including additional T cells, macrophages, and granulocytes. Consequently, the inflammatory lesions evolve into severe neurological dysfunctions such as ascending paraparesis and paralysis. Because the activated T cells are involved in the entire process, the trafficking of the activated MBP-specific T cells in EAE can reflect their immune activity in every evolutionary phase (2). Labeling T cells with imaging probes will allow non-invasive tracking of the migration of T cells in vivo.

The imaging probes can be internalized into cells with the use of cell-penetrating peptides (CPP) as vector/nuclear delivery vehicles of conjugated cargo (5). In general, CPP comprise a protein-transduction domain formed by small peptides (<20 amino acids) for cell membrane translocation. A commonly used CPP is a peptide truncated from the 86-mer transactivating transcriptional activator (Tat) protein in human immunodeficiency virus type 1 (HIV) (6). In particular, Tat(47-57) is widely used in cellular delivery of peptides, proteins, genetic material, antibodies, nanoparticles, and liposomes (5). Tat(47-57) contains an α-helical structure with a charged face formed by six arginine and two lysine residues (6). Tat-mediated internalization consists of multiple steps: the binding of Tat to the cell surface, stimulation of macropinocytotic uptake of Tat and transfer into macropinosomes, and finally endosomal escape into the cytoplasm (7).

A T lymphocyte is labeled with Cy5.5-Cys-Gly-Arg-Arg-Arg-Gln-Arg-Arg-Lys-Lys-Arg-Gly (CGRRRQRRKKRG) (Cy5.5-Tat-T cell) for optical imaging (2). This agent contains a near-infrared fluorescence (NIRF) dye shuttled across the cell membrane of T cells via Tat(48-57). The fluorescence probe Cy5.5 is a cyanine dye consisting of two quaternized heteroaromatic bases (A and A’) joined by a polymethine chain with five carbons (8), and it is bound to cysteine-terminated Tat(48-57) via a maleimide group as a spacer (2). Cy5.5 has a delocalized positive charge in its chromophore and possesses high quantum yield (0.22 at 678 nm), good chemical stability, easy conjugation, and high sensitivity (mole extinction coefficient ~250,000 mol/cm) (9, 10). The excitation/emission wavelength is 674/692 nm for Cy5.5, where hemoglobin and water have their lowest absorption coefficient. The labeled cargo Cy5.5-Tat is translocated through the plasma membrane of cells by an energy-dependent process involving endocytosis (2). The produced Cy5.5-Tat-T cells can be adoptively transferred to EAE rats for visualization and quantification of T cells activity in the early inflammation stages of EAE.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Cy5.5 + TAT + T cell)+AND+synthesis%0D%0A)]

Berger et al. briefly described the detailed preparation of Cy5.5-Tat-T cells (2). A cysteine-terminated Tat peptide (48-57) derived from 86-mer Tat protein (CGRRRQRRKKRG) was coupled with Cy5.5-maleimide (Cy5.5-Mal) in dimethyl sulfoxide at a ratio of 1:1. Then T cells were incubated with Cy5.5-Tat (molecular weight, 2596.1) at a concentration of 5–200 μg/ml overnight. The amount of Cy5.5-Tat peptide was estimated to be 5–50 pg per T cell as determined with in vitro measurement of Cy5.5 fluorescence. Cy5.5-Tat was found to be located predominantly in the cytoplasmic compartment of T cells.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Cy5.5 + TAT+ T cell)+AND+%22in+vitro%22)]

Berger et al. examined cell variability of Cy5.5-Tat-T cells in different culture media with fluorescent measurement (2). For media with 1–50 μg/ml of Cy5.5-Tat, the cell viability was not affected; however, for media with 100 and 200 μg/ml of Cy5.5-Tat, the surviving cells decreased by 10% to 30%, respectively. Berger et al. also performed a kinetic study on the labeling efficiency. T cells were incubated with 200 μg/ml Cy5.5-Tat for different durations. Incubation for 1 h generated ~19.5% labeled living cells. This fraction increased to 36.4% with 12 h of incubation, including 12.7% of CD4^+^ and 23.7% of CD8^+^ cells. Even with such a long incubation time, approximately one third of the total T cells were not labeled. These cells either did not favor Tat peptide mediation of cell penetration or the labels were degraded in these cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Cy5.5 + TAT+ T cell) +AND++rodentia)]

Berger et al. used in vivo NIRF imaging to study the filtration of Cy5.5-Tat-T cells into the central nervous systems of EAE rats (2). Lewis rats with chronic relapsing EAE were used in the study to provide different patterns of neurological impairment during the acute phase (10–12 days postimmunization (dpi) against myelin), the remitting phase (15–20 dpi), and first relapse phase (21–26 dpi). Activated Cy5.5-Tat-T cells (~10^7^ cells) were adoptively transferred intravenously at 5, 7, and 11 dpi followed by NIFR imaging up to 22 dpi. In all rats, an intense fluorescence signal was found in the brain immediately after injection of the activated Cy5.5-Tat-T cells. Pronounced variations in the different phases of the disease were observed; i.e., EAE rats injected with activated Cy5.5-Tat-T cells at 7 dpi demonstrated an increase in fluorescence before the onset of symptoms (9 dpi): the strongest intensity (~90% of its initial value) was observed at the end of the acute phase (15 dpi); a decrease to 32% was observed at remitting phase (19 dpi); and an increase to 50% was observed at relapsing phase (22 dpi). This alteration reflected the accumulation of activated Cy5.5-Tat-T cells in the inflammation sites, which triggered the infiltration of activated monocytes generated at the lesions and increased the recruitment for activated Cy5.5-Tat-T cells in the immune reaction against myelin. As controls, healthy rats received the activated Cy5.5-Tat-T cells, naïve Cy5.5-Tat-T cells, or Cy5.5-Tat. An intense fluorescence signal was also found in the brain immediately after injection in these rats, but the intensity decreased to baseline level within 1 day and remained constant at much lower intensity levels at all other time points. Only the healthy rats injected with activated Cy5.5-Tat-T cells at 7 dpi had intensity of ~50% of its initial value during 12–15 dpi, which decreased subsequently to 32%.

Berger et al. confirmed the presence of Cy5.5-Tat-T cells in the lesions of EAE rats ex vivo (2). Fluorescence microscopy was used to examine the excised brain slices at 12 dpi and 22 dpi. Significant amounts of Cy5.5 were found in all EAE rats and in the healthy rats that were injected with activated Cy5.5-Tat-T cells. As controls, EAE rats injected with non-activated Cy5.5-Tat-T cells or healthy rats injected with activated Cy5.5-Tat-T cells exhibited significantly weaker fluorescence or absence of fluorescence. The slices from EAE rats were further examined with immunohistochemical stains to identify T lymphocytes with CD3 tracers and macrophages with ED2 tracers (2). The exact co-localization of CD3 and ED2 tracers in the periphery of the medulla confirmed the predominant infiltration of these cells into EAE lesions. Confocal images demonstrated that both the T lymphocytes and macrophages were labeled with Cy5.5-Tat, indicating the phagocytosis of Cy5.5-Tat-T cells by activated monocytes.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Cy5.5 + TAT+ T cell) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Cy5.5 + TAT+ T cell) +AND+human)]

No publication is currently available.

## References

1 Hohlfeld R. Meinl E. Weber F. Zipp F. Schmidt S. Sotgiu S. Goebels N. Voltz R. Spuler S. Iglesias A. The role of autoimmune T lymphocytes in the pathogenesis of multiple sclerosis Neurology 1995 45Suppl 66 S33 8 7783909
2 Berger C., Gremlich H.U., Schmidt P., Cannet C., Kneuer R., Hiestand P., Rausch M., Rudin M. (2007). In vivo monitoring the fate of Cy5.5-Tat labeled T lymphocytes by quantitative near-infrared fluorescence imaging during acute brain inflammation in a rat model of experimental autoimmune encephalomyelitis. J Immunol Methods.
3 Wekerle H., Kojima K., Lannes-Vieira J., Lassmann H., Linington C. (1994). Animal models. Ann Neurol.
4 Gold R., Linington C., Lassmann H. (2006). Understanding pathogenesis and therapy of multiple sclerosis via animal models: 70 years of merits and culprits in experimental autoimmune encephalomyelitis research. Brain.
5 Berry C.C. (2008). Intracellular delivery of nanoparticles via the HIV-1 tat peptide. Nanomed.
6 Torchilin V.P. (2008). Tat peptide-mediated intracellular delivery of pharmaceutical nanocarriers. Adv Drug Deliv Rev.
7 Gump J.M., Dowdy S.F. (2007). TAT transduction: the molecular mechanism and therapeutic prospects. Trends Mol Med.
8 Ernst L.A., Gupta R.K., Mujumdar R.B., Waggoner A.S. (1989). Cyanine dye labeling reagents for sulfhydryl groups. Cytometry.
9 Ballou B., Fisher G.W., Hakala T.R., Farkas D.L. (1997). Tumor detection and visualization using cyanine fluorochrome-labeled antibodies. Biotechnol Prog.
10 Lin Y., Weissleder R., Tung C.H. (2002). Novel near-infrared cyanine fluorochromes: synthesis, properties, and bioconjugation. Bioconjug Chem.